# Gadobenate

Chemical name: | Gadobenate
Abbreviated name: | Gd-BOPTA
Synonym: | MultiHance®, B-19036, Gd-BOPTA/Dimeg, gadobenate dimeglumine, (4RS)-[4-carboxy-5,8,11-tris(carboxymethyl)-1-phenyl-2-oxa-5,8,11-triazatridecan-13-oato(5-)]gadolinate (2-) dihydrogen with 1-deoxy-1-(methylamino)-D-glucitol (1:2)
Agent Category: | Compound
Target: | Non-targeted, CNS
Target Category: | Blood-brain barrier breakdown
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/ contrast: | Gadolinium (Gd)
Activation: | No
Studies: | - In vitro; - Rodents; - Other non-primate mammals; - Non-human primates; - Humans | Structure of Gadobenate.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Gadobenate%20or%20Gd-BOPTA%20or%20MultiHance%22)]

Gadobenate (Gd-BOPTA) is a paramagnetic contrast agent for magnetic resonance imaging (MRI) that was approved by the United States Food and Drug Administration (US FDA) in 2004 for imaging the central nervous system to visualize lesions with abnormal blood-brain barrier (BBB) or abnormal vascularity of the brain, spine, and associated tissues (1-3).

Conventional, water-soluble, paramagnetic contrast agents are generally metal chelates with unpaired electrons, and they work by shortening both T_1_ and T_2_ relaxation times of surrounding water protons to produce the contrast-enhancing effect (1, 2). At normal clinical doses, the T_1_ effect tends to dominate. Current agents are water-soluble compounds that distribute in the extracellular fluid and do not cross the intact BBB. They can be used to enhance signals of CNS tissues that lack a BBB (e.g., pituitary gland), extraaxial tumors (e.g., meningiomas), and areas of BBB breakdown (e.g., tumor margins). In these cases, small or multiple CNS lesions are more clearly delineated with contrast enhancement. In addition, contrast enhancement can highlight vasculature, delineate the extent of disease, and confirm the impression of normal or nonmalignant tissues. These contrast agents can also be used in a similar nonspecific manner to enhance contrast between perfused and nonperfused areas in other organs (1, 2, 4).

Gadolinium ion (Gd^3+^), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective at enhancing proton relaxation because of its high magnetic moment and very labile water coordination (2, 5-7). Gadopentetate dimeglumine (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar gadolinium chelates have been developed in an effort to further improve clinical efficacy, patient safety and patient tolerance. The major chemical differences among these Gd chelates or Gd-based contrast agents (GBCAs) are the presence or absence of overall charge, ionic or nonionic, and their ligand frameworks (linear or macrocyclic). Gd-BOPTA has a linear framework and is ionic. The BOPTA ligand was originally developed as a potential hepatobiliary agent for MRI (8). It is a modification of the DTPA molecule based on the belief that the addition of a benzoylmethyl group to the backbone of DTPA would increase the liver uptake of Gd-BOPTA. The hepatobiliary excretion of Gd-BOPTA appears to be species dependent, and only 2-5% of the dose is excreted via the biliary system in humans. Because of weak/transient interactions between Gd-BOPTA and macromolecules that reduce the tumbling rate of the Gd-BOPTA molecules, Gd-BOPTA demonstrates increased r_1_ and r_2_ relaxivities (efficiencies in shorteningT_1_ and T_2_ relaxation times) in solutions containing serum proteins (9-11).

The commercial formulation (http://multihanceusa.com/packageinserts.htm) of Gd-BOPTA is a meglumine salt (Gd-BOPTA/Dimeg) and is available as a 0.5 M injection with a recommended dose of 0.1 mmol/kg (0.2 ml/kg) either as a rapid intravenous infusion or bolus injection for CNS MRI imaging (3, 12). It has an osmolality of 1970 osmol/kg and viscosity of 5.3 mPas at 37^o^C.

Both renal and extra-renal toxicities have been reported following the clinical use of gadolinium in patients with underlying kidney disease (13-15). In 2007, the US FDA (http://www.fda.gov/cder/drug/infopage/gcca/default.htm) requested manufacturers of all GBCAs to add new warnings about exposure to GBCAs increases the risk for nephrogenic systemic fibrosis (NSF) in patients with advanced kidney disease.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28BOPTA%20or%20Gd-BOPTA%20or%20gadobenate%20or%20B-19036%29%20AND%20synthesis)]

Felder et al. (16) first synthesized the BOPTA ligand in 1987. Uggeri et al. (17) reported that the synthesis of BOPTA consisted of two major steps. Diethylenetriamine was first selectively monoalkylated on a primary amino group with 2-chloro-3-(phenylmethoxy)propanoic acid in water at 50^o^C for 40 h. The intermediate product was isolated as N-[2-[(2-aminoethyl)amino]ethyl]-O-(phenylmethyl)-DL-serine tris-(hydrochloride) with the yield of 58%. This intermediate compound was then fully carboxymethylated with bromoacetic acid in water at pH 10 and room temperature for 15 h, and the yield of BOPTA was 21%. Gd-BOPTA dimeglumine salt was prepared by mixing BOPTA with N-methylglucamine and Gd_2_O_3_ at 80^o^C for 1.5 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28BOPTA%20or%20Gd-BOPTA%20or%20B-19036%20or%20gadobenate%20or%20MultiHance%29%20AND%20in%20vitro)]

In in vitro studies, Gd-BOPTA/Dimeg at a concentration of 30 mM caused a slight reduction of the contractile force in a rat papillary muscle preparation, and a mild decrease of both amplitude and contraction rate in isolated guinea pig atria (18).

The water proton relaxation of Gd-BOPTA in a protein-free aqueous solution was measured at 20 MHz, 39^o^C and pH 7.4, and its longitudinal (r_1_) and transverse (r_2_) relaxivities values in mM−^1^S−^1^were reported to be 4.39 ± 0.01 and 5.56 ± 0.02, respectively (11, 17). The conditional stability constant (log K*_ML_) of Gd-BOPTA determined by competition complexation experiments was 18.4 at pH 7.4 and 20^o^C. The r_1_ relaxivity of Gd-BOPTA in heparinzed human plasma was reported to be 9.7 mM−^1^S−^1^. Cavagna et al. (19) reported that no binding of Gd-DOPTA/Dimeg to serum proteins could be detected using equilibrium dialysis (detection sensitivity at equilibrium constants = or < 5 mM) against rat, rabbit, or human plasma. With the use of different bovine serum albumin (BSA) concentrations, an in vitro nuclear magnetic relaxation dispersion (NMRD) profile of Gd-BOPTA/Dimeg was constructed to show that protein concentrations had a strong influence on Gd-BOPTA/Dimeg relaxivity (20).

Caravan et al. (21) in a 2003 study found that the ion-nuclear distance of Gd to a coordinated water proton, r_Gd-H_, was 3.1 ± 0.1 Å for Gd-BOPTA and four other Gd complexes. Partition coefficients of Gd-BOPTA/Dimeg in the systems of n-butanol or n-octanol with 0.01 M phosphate buffer pH 7.3 were found to be 0.0067 and 0.0016, respectively (22).

Planchamp et al. (23) used a hollow-fiber bioreactor to study the transport of Gd-BOPTA/Dimeg into rat hepatocytes. They reported that the results supported a transporter-mediated mechanism, and the Michaelis-Menton constant (K_m_) was estimated to be 270 µM. In another isolated rat liver study, the uptake of Gd-BOPTA into hepatocytes and its subsequent biliary excretion appeared to be highly temperature dependent (24).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28BOPTA%20or%20B-19036%20or%20gadobenate%20or%20MultiHance%20or%20Gd-BOPTA%29%20AND%20rodentia)]

In rats, Gd-BOPTA/Dimeg rapidly distributed in the extravascular and extracellular compartments, and it showed a marked affinity for biliary excretion (19, 25). The biodistribution study showed that Gd-BOPTA/Dimeg was found mainly in the liver and kidney. Vittadini et al. (26) conducted pharmacokinetic studies of Gd-BOPTA/Dimeg (0.05 mmol/kg) in rats and found that the blood kinetics (distribution t_½_, elimination t_½_ and apparent volume of distribution V_d_) and excretion kinetics of 6 h (total clearance, urinary excretion and biliary excretion) were 3.8 ± 0.5 min, 15.05 ± 0.54 min, 165.1 ml/kg and 13.9 ml/min/kg, 54.8 ± 8.8% injected dose (ID), 38.6 ± 7.3% ID, respectively. Cavagna et al. (19) reported that the bile and urine eliminations of Gd-BOPTA in rats at 8 h were 52% ID and 46% ID, respectively. There was no or weak binding of Gd-BOPTA/Dimeg to plasma proteins and no apparent biotransformation of the compound.

The acute i.v. LD_50_ of Gd-BOPTA/Dimeg in rats was 6.6 (5.8-7.5, n = 5) mmol/kg at 6 ml/min and 9.2 (8.1-10.4) mmol/kg at 0.2 ml/min (27). No observed effect levels (NOEL) were observed in rats with repeated doses up to 0.3 mmol/kg/day. Only a mild and transient reduction in heart rate was observed at the dose of 1 mmol/kg (18). Luzzani et al (28). studied the brain penetration and neurological effects of Gd-BOPTA in rats with various i.v. and intracisternal injection doses of ^153^Gd-BOPTA. At 0.01 mmol/kg of intracisternal injection of ^153^Gd-BOPTA/Dimeg, the motor coordination was slightly impaired. No neurological effect was observed with i.v. doses of ^153^Gd-BOPTA up to 2 mmol/kg. Noce et al. (29)did not find any effect of Gd-BOPTA on cerebral glucose metabolism after an intracerebral dose of 120 nmol/rat. In the same study, no genotoxic potential was observed in mutagenicity tests, and the reproductive performance and development of offspring were not affected at doses up to 20 times the human dose.

The acute i.v. LD_50_ of Gd-BOPTA/Dimeg in mice was 5.7 (5.3-6.2, n = 5) mmol/kg at 6 ml/min and 7.9 (7.5-8.3) mmol/kg at 0.2 ml/min (27). The intracerebral LD_50_ was 1.02 mmol/kg (26). In another preclinical study in rats, Gd-BOPTA/Dimeg at the i.v. dose of 1 mmol/kg caused a decrease of blood pressure of about 15%, a decrease of heart rate of about 7%, but no significant ECG alterations (22).

With the use of MRI imaging (2 Tesla, T_1_-weighted), in vivo relaxivity (r_1_) values of Gd-BOPTA/Dimeg (200 µmol/kg) in the blood, normal and infracted myocardium of rats were determined to be 6.19, 4.05, and 10.03 mM−^1^s−^1^, respectively (20). In comparison, the corresponding values for Gd-DTPA were reported to be 3.41, 3.52, and 5.32 mM−^1^s−^1^.

Pastor et al. (30) studied the hepatic kinetics of Gd-BOPTA/Dimeg with the use of MRI (1.5 Tesla, T_1_-weighted) in a perfused rat liver model. They found that the hepatic activity uptake t_½_ was 4.8 ± 0.3 min, and the washout t_½_ was 17.5 ± 2.8 min.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gd-BOPTA%20or%20BOPTA%20or%20gadobenate%20or%20MultiHance%20or%20B-19036%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Lorusso and colleagues showed that Gd-BOPTA/Dimeg distributes into plasma, extracellular fluid, and intrahepatocytic space in both rabbits and dogs (25). Gd-BOPTA was not metabolized and was cleared from plasma by renal and biliary excretion.

Morisetti et al. (27) found no adverse effects of Gd-BOPTA/Dimeg treatment on rabbit dams or on fetuses at a dose of 0.3 mmol/kg per day. Cavagna et al. (19) used MRI (2 Telsa, T_1_-weighted) to perform the in vivo determination of the relaxation rate of Gd-BOPTA/Dimeg (0.1 mmol/kg) in rabbit blood. The longitudinal relaxation rate was 1.93 ± 0.06 s−^1^ at 5 min after injection.

No significant cardiovascular and respiratory effects of Gd-BOPTA/Dimeg at i.v. dose of 1 mmol/kg (10 ml/min) in Large White pigs (18). In a myocardial ischemia Yucatan micropig model, i.v. doses of Gd-BOPTA/Dimeg up to 3 mmol/kg did cause dose-dependent cardiovascular changes.

Port and colleagues (31) used a rabbit experimental model to determine that the dynamic relaxivity (r_1dynamic_) of Gd-BOPTA in plasma was 5.2 mM−^1^s−^1^ (60 MHz) at the bolus phase (0-15 sec postinjection) when 93% of Gd-BOPTA was present in the free form. The r_1dynamic_ was 6.7 mM−^1^s−^1^ at the postbolus phase (1-5 min postinjection) when 82% of Gd-BOPTA remained in the free form.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gd-BOPTA%20or%20BOPTA%20or%20MultiHance%20or%20gadobenate%20or%20B-19036%29%20AND%20%28primate%20NOT%20human%29)]

The NOEL dose of Gd-BOPTA/Dimeg was found to be 0.25 mmol/kg/day (i.v.) in Cynomolgus monkeys (27) In the doses ranging from 0.25 to 3 mmol/kg, the maximal plasma concentration and the area under the plasma concentration-time curve were linearly related to the dose (25). Runge (32) studied MRI (1.5 Tesla, T_1_-weighted) of Gd-BOPTA/Dimeg at the dose of 0.1 mmol/kg in rhesus monkeys (n = 4). The enhancements (percent increase in signal intensity before injection) of the muscle, kidneys, and spleen were maximum at 2 min (40 ± 17%), 5 min (164 ± 25%), and 5 min (92 ± 25%) after injection, respectively. Two peaks of liver enhancement were observed with 114 ± 45% occurred immediately and then with 136 ± 23% occurred at 30 min after injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gd-BOPTA%20or%20BOPTA%20or%20MultiHance%20or%20gadobenate%20or%20B-19036%29%20AND%20human)]

The Phase I study by Spinazzi et al. (33) and the Phase II clinical trial by Rosati et al (34). reported the safety and pharmacokinetics data of Gd-BOPTA/dimeg. The pharmacokinetics profile was studied in 28 healthy volunteers. Gd-BOPTA/Dimeg was given in seven different i.v. doses ranging from 0.05 mmol/kg to 0.4 mmol/kg. In the dose range from 0.005 mmol/kg to 0.2 mmol/kg, the pharmacokinetics value ranges (n = 4) of the distribution t_½_, elimination t_½_, V_d_, and the total clearance (CL) were 0.084-0.36 h, 1.17-1.68 h, 0.074-0.142 liter/kg, 0.170-0.248 liter/kg, and 0.098-0.133 liter/h/kg, respectively. In the dose range from 0.2 mmol/kg to 0.4 mmol/kg, the value ranges (n = 4 ) of the distribution t_½_, elimination t_½_, V_d_, and CL were 0.48-0.605 h, 1.95-2.02 h, 0.147-0.158 liter/kg, 0.261-0.282 liter/kg, and 0.093-0.098 l/h/kg, respectively. In 72 h, 89-95.2% of the injected dose was eliminated unchanged by the kidneys and about 0.6-3.5% was excreted in the bile. With the use of equilibrium dialysis, the complex did not appear to bind measurably to plasma proteins. Safety studies in 39 volunteers indicated an18% of adverse events as compared with 14% in the placebo group (n = 14). The most frequent adverse events were altered sensation at the injection site, nausea, and sweating. In 127 patients with intracranial lesions, Gd-BOPTA/Dimeg (0.1-0.2 mmol/kg) provided better diagnostic information in 95% of the cases than those of MRI without contrast.

Phase III double-blind, multicenters (28 centers), randomized, parallel group comparative studies with 410 CNS patients had shown that Gd-BOPTA/Dimeg at doses of 0.05-0.15 mmol/kg and 0.1-0.2 mmol/kg had comparable safety and efficacy profiles as Gd-DTPA-BMA at doses of 0.1 mmol/kg and 0.3 mmol/kg for imaging of CNS lesions (35, 36). Other studies had investigated the potential usefulness of Gd-BOPTA/Dimeg for liver imaging [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gd-BOPTA%20or%20BOPTA%20or%20MultiHance%20or%20gadobenate%20or%20B-19036%29%20AND%20liver%20imaging%20in%20humans)] and magnetic resonance angiography [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gd-BOPTA%20or%20BOPTA%20or%20MultiHance%20or%20gadobenate%20or%20B-19036%29%20AND%20angiography)].

## Supplemental Information

[Disclaimers]

Gadobenate package insert

Gadobenate multipack package insert

## References

1 Brasch RC, Ogan MD, Engelstad BL. Paramagnetic Contrast Agents and Their Application in NMR Imaging, in Contrast media; Biologic effects and clinical application, Z. Parvez, R., R. Monada and M. Sovak, Editor. 1987, CRC Press, Inc.: Boca Raton, Florida. p. 131-143.
2 Saini S, Ferrucci JT. Enhanced Agents for Magnetic Resonance Imaging: Clinical Applications, in Pharmaceuticals in Medical Imaging, D.P. Swanson, H.M. Chilton and J.H. Thrall, Editor. 1990, MacMillan Publishing Co., Inc.: New York. p. 662-681.
3 multihance (gadobenate dimeglumine injection, 529 mg/ml) Package Insert. 2005: Bracco Diagnostics Inc. F1/3.541037.
4 Runge V., Kirsch J., Wells J., Awh M., Bittner D., Woolfolk C. (1993). Enhanced liver MR: Contrast agents and imaging strategy. Crit Rev Diagn Imaging.
5 DeSimone D., Morris M., Rhoda C., Lucas T., Zielonka J., Olukotun A., Carvlin M. (1991). Evaluation of the safety and efficacy of gadoteridol injection (a low osmolal magnetic resonance contrast agent). Clinical trials report. Invest Radiol.
6 Tweedle M. (1992). Physicochemical properties of gadoteridol and other magnetic resonance contrast agents. Invest Radiol.
7 Yuh W., Engelken J., Muhonen M., Mayr N., Fisher D., Ehrhardt J. (1992). Experience with high-dose gadolinium MR imaging in the evaluation of brain metastases. AJNR Am J Neuroradiol.
8 Oksendal A., Hals P. (1993). Biodistribution and toxicity of MR imaging contrast media. J Magn Reson Imaging.
9 Kirchin M., Pirovano G., Spinazzi A. (1998). Gadobenate dimeglumine (Gd-BOPTA). An overview. Invest Radiol.
10 Essig M. (2005). Gadobenate dimeglumine (MultiHance) in MR imaging of the CNS: studies to assess the benefits of a high relaxivity contrast agent. Acad Radiol.
11 de Haen C., Cabrini M., Akhnana L., Ratti D., Calabi L., Gozzini L. (1999). Gadobenate dimeglumine 0.5 M solution for injection (MultiHance) pharmaceutical formulation and physicochemical properties of a new magnetic resonance imaging contrast medium. J Comput Assist Tomogr.
12 de Haen C., Gozzini L. (1993). Soluble-type hepatobiliary contrast agents for MR imaging. J Magn Reson Imaging.
13 Perazella M.A., Rodby R.A. (2007). Gadolinium use in patients with kidney disease: a cause for concern. Semin Dial.
14 Grobner T., Prischl F.C. (2007). and Gadolinium and nephrogenic systemic fibrosis. Kidney Int.
15 Pedersen M. (2007). Safety update on the possible causal relationship between gadolinium-containing MRI agents and nephrogenic systemic fibrosis. J Magn Reson Imaging.
16. Felder, E., R. Vitale, F. Uggeri, L. Fumagalli, and G. Vittadini, 1990.
17 Uggeri F., Aime S., Anelli P., Botta M., Brocchetta M., de Haen C., Ermondi G., Grandi M., Paoli P. (1995). Novel contrast agents for magnetic resonance imaging. Synthesis and characterization of the ligand BOPTA and its Ln(III) complexes (Ln=Gd, La, Lu). X-ray structure of disodium (TPS-9-145337286-C-S)-[4-carboxy-5,8,11-tris(carboxymethyl)-1-phenyl-2-oxa-5,8,11-triazatridecan-13-oato(5-)]gadolinate(2-) in a mixture with its enantiomer. Inorg Chem.
18 Tirone P., Castano M., Cipolla P., Frigeni V., La Noce A., Luzzani F., Valenti R., de Haen C. (1999). General pharmacology in experimental animals of gadobenate dimeglumine (MultiHance), a new magnetic resonance imaging contrast agent. J Comput Assist Tomogr.
19 Cavagna F., Maggioni F., Castelli P., Dapra M., Imperatori L., Lorusso V., Jenkins B. (1997). Gadolinium chelates with weak binding to serum proteins. A new class of high-efficiency, general purpose contrast agents for magnetic resonance imaging. Invest Radiol.
20 Cavagna F., Marzola P., Dapra M., Maggioni F., Vicinanza E., Castelli P., de Haen C., Luchinat C., Wendland M., Saeed M., Higgins C. (1994). Binding of gadobenate dimeglumine to proteins extravasated into interstitial space enhances conspicuity of reperfused infarcts. Invest Radiol.
21 Caravan P., Astashkin A., Raitsimring A. (2003). The gadolinium(III)-water hydrogen distance in MRI contrast agents. Inorg Chem.
22 Vittadini G., Felder E., Musu C., Tirone P. (1990). Preclinical profile of Gd-BOPTA. A liver-specific MRI contrast agent. Invest Radiol.
23 Planchamp C., Ivancevic M., Pastor C., Vallee J., Pochon S., Terrier F., Mayer J., Reist M. (2004). Hollow fiber bioreactor: new development for the study of contrast agent transport into hepatocytes by magnetic resonance imaging. Biotechnol Bioeng.
24 Planchamp C., Beyer G., Slosman D., Terrier F., Pastor C. (2005). Direct evidence of the temperature dependence of Gd-BOPTA transport in the intact rat liver. Appl Radiat Isot.
25 Lorusso V., Arbughi T., Tirone P., de Haen C. (1999). Pharmacokinetics and tissue distribution in animals of gadobenate ion, the magnetic resonance imaging contrast enhancing component of gadobenate dimeglumine 0.5 M solution for injection (MultiHance). J Comput Assist Tomogr.
26 Vittadini G., Felder E., Tirone P., Lorusso V. (1988). B-19036, a potential new hepatobiliary contrast agent for MR proton imaging. Invest Radiol.
27 Morisetti A., Bussi S., Tirone P., de Haen C. (1999). Toxicological safety evaluation of gadobenate dimeglumine 0.5 M solution for injection (MultiHance), a new magnetic resonance imaging contrast medium. J Comput Assist Tomogr.
28 Luzzani F., Cipolla P., Pelaprat M., Robert F., Gotti C., Tirone P., de Haen C. (1997). Brain penetration and neurological effects of gadobenate dimeglumine in the rat. Acta Radiol.
29 La Noce A., Frigeni V., Filatori I., Danieli A., Tirone P. (2000). Gadobenate dimeglumine and cerebral glucose metabolism. Continuous monitoring of striatal lactate levels in freely moving rats. Acta Radiol.
30 Pastor C., Planchamp C., Pochon S., Lorusso V., Montet X., Mayer J., Terrier F., Vallee J. (2003). Kinetics of gadobenate dimeglumine in isolated perfused rat liver: MR imaging evaluation. Radiology.
31 Port M., Corot C., Violas X., Robert P., Raynal I., Gagneur G. (2005). How to compare the efficiency of albumin-bound and nonalbumin-bound contrast agents in vivo: the concept of dynamic relaxivity. Invest Radiol.
32 Runge V. (1998). A comparison of two MR hepatobiliary gadolinium chelates: Gd-BOPTA and Gd-EOB-DTPA. J Comput Assist Tomogr.
33 Spinazzi A., Lorusso V., Pirovano G., Kirchin M. (1999). Safety, tolerance, biodistribution, and MR imaging enhancement of the liver with gadobenate dimeglumine: results of clinical pharmacologic and pilot imaging studies in nonpatient and patient volunteers. Acad Radiol.
34 Rosati G., Pirovano G., Spinazzi A. (1994). Interim results of phase II clinical testing of gadobenate dimeglumine. Invest Radiol.
35 Runge V., Armstrong M., Barr R., Berger B., Czervionke L., Gonzalez C., Halford H., Kanal E., Kuhn M., Levin J., Low R., Tanenbaum L., Wang A., Wong W., Yuh W., Zoarski G. (2001). A clinical comparison of the safety and efficacy of MultiHance (gadobenate dimeglumine) and Omniscan (Gadodiamide) in magnetic resonance imaging in patients with central nervous system pathology. Invest Radiol.
36 Runge V., Parker J., Donovan M. (2002). Double-blind, efficacy evaluation of gadobenate dimeglumine, a gadolinium chelate with enhanced relaxivity, in malignant lesions of the brain. Invest Radiol.